# Alexa Fluor 680-NH-CO-CH_2_-S-CH_2_-Phe-Pro-Arg-CH_2_-prothrombin

Chemical name: | Alexa Fluor 680-NH-CO-CH_2_-S-CH_2_-Phe-Pro-Arg-CH_2_-prothrombin
Abbreviated name: | AF680-ProT
Synonym:
Agent Category: | Proteins
Target: | Staphylocoagulase
Target Category: | Bacterial enzyme
Method of detection: | Optical imaging
Source of signal / contrast: | Alexa Fluor 680
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Staphylococcus%20aureus%20endocarditis%20and%20%20imaging)]

The fluorescently labeled prothrombin analog, Alexa Fluor 680-NH-CO-CH_2_-S-CH_2_-Phe-Pro-Arg-CH_2_-prothrombin, abbreviated as AF680-ProT, is a probe developed by Panizzi et al. for detecting Staphylococcus aureus (S. aureus) endocarditis by targeting staphylocoagulase (1).

Infective endocarditis is a life-threatening condition that is commonly caused by S. aureus, and the hallmark of S. aureus endocarditis is the development of vegetations on heart valves (2). After entering into the bloodstream, S. aureus proliferates quickly, colonizes on either damaged or normal heart valves, and leads to a rapid progressive endocarditis with destruction of the heart valves (3-5). In this pathological process, adherence of S. aureus to heart valves is the key to initiate the vegetation formation, and SC is one of the most important stimulators of the initiation. SC is an extracellular protein secreted by coagulase-positive S. aureus, and it can bind prothrombin with a high affinity (K_d_ = ~17–72 pM) in a 1:1 stoichiometry (6-8). This binding forms an active SC-prothrombin complex, which induces plasma coagulation via specific cleavage of fibrinogen to fibrin (7, 9). The N-terminal D1 and D2 regions of SC are involved in the binding with prothrombin and its activation, and the C-terminal repeat region, comprising 27-amino-acid tandem repeats, is associated with the adherence of SC to fibrinogen (10, 11).

Panizzi et al. synthesized an engineered analog of human prothrombin in which the active site was modified by a thrombin inhibitor that possesses a protected thiol group (1, 6). Thus, the prothrombin analog could react with a thiol-specific Alexa Fluor 680 dye (AF680-ProT) for fluorescence imaging or with diethylenetriamine pentaacetic acid (DTPA) for ^64^Cu-labeling (^64^Cu-DTPA-ProT). The rationale underlying this design is the SC-dependent prothrombin recruitment, which simultaneously tethers the active SC-prothrombin analog complex into the fibrin(ogen)-rich S. aureus vegetations. Imaging studies by Panizzi et al. showed that the two probes could bind SC and intercalate into growing bacterial vegetations on the heart valves, with the potential to detect S. aureus endocarditis and monitor antibiotic therapy via noninvasive optical imaging and positron emission tomography (1).

This chapter summarizes the data obtained with AF680-ProT, and another chapter summarizes the data obtained with ^64^Cu-DTPA-ProT.

### Related Resource Links:

The nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/?term=staphylocoagulase) and protein (http://www.ncbi.nlm.nih.gov/protein?term=staphylocoagulase) sequences of staphylocoagulase in GenBank

The structure of staphylocoagulase (http://www.ncbi.nlm.nih.gov/structure?term=staphylocoagulase)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21857652)]

Panizzi et al. described the synthesis of AF680-ProT in detail (1, 6). Prothrombin was purified from human plasma (absorption coefficient, 1.47 (mg/ml)−^1^cm−^1^; molecular weight, 71.6 kDa). Met-SC-(1–325)-His_6_ fragment was expressed in E. coli strain BL21(DE3) plysS and purified from the soluble fraction after centrifugation. An active site was first induced through the binding of Met-SC-(1–325)-His_6_ with prothrombin. This site was then inactivated via Ser^195^ and His^57^ alkylation with the thiol group-possessing thrombin inhibitor N^α^-[(acetylthio)acetyl]-D-Phe-Pro-Arg-CH_2_Cl (ATA-FPR-CH_2_Cl). The resulting Met-SC-(1–325)-His_6_·ATA-FPR-ProT complex was fluorescently labeled through the reaction with a 10-fold molar excess of thiol-reactive Alexa Fluor 680 C_2_ maleimide. Finally, the Met-SC-(1–325)-His_6_ was dissociated with NaSCN from the fluorescently labeled complex, and the desired product, AF680-ProT, was separated with gel filtration chromatography. The chemical purity of AF680-ProT and the number of dye moieties per probe were not described in detail.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21857652)]

Panizzi et al. first determined the activity of the residual active prothrombin in the final product because the residual active prothrombin could trigger downstream activation of the clotting cascade in vivo (1). The results showed a residual activity of 0.3% for AF680-ProT, indicating less potential to trigger clotting cascade when used in vivo.

Panizzi et al. then verified whether the recombinant N-terminal fragment SC (1–325) was able to activate mouse prothrombin. The investigators found that the SC (1–325)-prothrombin complex hydrolyzed the chromogenic substrate of H-D-Phe-Pip-Arg-pNA (S2238) at a rate that was equivalent to that of mouse thrombin (k_cat_ = 26 ± 1 s−^1^) (1, 6). The supernatants of various S. aureus strains were able to clot mouse plasma. These data indicate that the mouse is an appropriate model organism to study SC function and regulation in vivo.

To determine the molecular mechanism underlying prothrombin recruitment to vegetations, Panizzi et al. performed in vitro native gel binding experiments using either the N-terminal active fragment SC (1–325) or the full-length SC (1–660) (1, 6). After incubation of these SC forms with prothrombin and fibrinogen fragment D (FragD), SC (1–325) and prothrombin bound together but lacked the ability to interact with FragD. However, SC (1–660) formed an SC-prothrombin-FragD ternary complex, and multiple FragD subunits interacted with a single SC molecule. The SC recombinant fragment that contained only the pseudorepeat and the first SC repeat could bind FragD with a K_d_ of 36 ± 8 nM. These results suggest that SC could interact with at least four fibrinogen or fibrin molecules per SC molecule to form a megaprotein complex, and this complex anchored the active SC-prothrombin complex to the growing vegetation.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21857652)]

To test the feasibility of AF680-ProT to image vegetations, Panizzi et al. established several mouse models of infective endocarditis by inserting a segment of suture material down the right carotid artery into the heart to induce damage of the aortic valve and by injecting bacteria (1 × 10^6^ colony-forming units per 100 ìl phosphate-buffered saline (PBS)) via the tail vein 24 h later (1). Bacterial strains used to establish disease models included SC-positive S. aureus strains (Newman D2 Tager 104, Xen29, and Xen8.1), SC-negative S. epidermidis FDA strain PCI 1200, and Newman SC and von Willebrand factor–binding protein (vWbp) double-knockout S. aureus (n = 6 mice/group). Newman D2 Tager 104, Xen29, and Xen8.1 are vancomycin-susceptible. Endocarditis was observed in >85% of the mice, but the size of formed vegetations and the extent of occlusion of the aortic valve varied, potentially correlating with the extent of denuded endothelium caused by the mechanical injury. On day 2 after suture insertion and 24 h after induction of bacteremia, 30–45 ìg AF680-ProT was injected via the tail vein, and imaging was performed 24 h later with fluorescence molecular tomography fused to X-ray computed tomography (FMT-CT). The isotropic spatial resolution was 110 ìm for CT and 1 mm for FMT.

FMT-CT imaging showed that AF680-ProT accumulated in the vegetations, which was consistent in mice induced with Tager 104, Xen29, and Xen8.1 strains, but not in mice infected with S. epidermidis or in mice without bacteremia. The fluorescence intensity in the aortic outflow tract in mice with S. aureus–induced vegetations was 20- to 28-fold higher than that in the mice without bacteremia and the mice with S. epidermidis challenge (1). AF680-ProT had a blood half-life of 79 ± 14 min.

The expression pattern of SC within vegetations was investigated in the excised aortas with vegetations (1). AF680-ProT was co-localized with SC at the interface of vegetations with the host's circulation, although bacteria were present throughout the vegetations. This result was consistent with the findings from immunoreactive staining for SC and vWbp and from in situ hybridization for SC RNA, which showed that the proteins and RNA were all limited to the periphery of vegetations. This SC expression pattern was considered to be the result of the differential expression of SC during vegetation development; as in younger lesions with lower bacterial burden, the entire S. aureus population stained positive for SC.

To image the efficiency of AF680-ProT for monitoring vancomycin therapy, mice were given daily intraperitoneal injections of 10 ìg vancomycin or PBS for 6 days (n = 8–10 mice/group) (1). FMT-CT imaging at 48 h after infection indicated that AF680-ProT was able to quantify the effect of vancomycin, showing that vancomycin treatment eliminated bacteria in vegetations and that termination of the therapy resulted in recurrence of the infection and a high risk of mortality, similar to the relapse observed in some patients with infective endocarditis.

To determine the specificity of AF680-ProT for endocarditic vegetations that contain SC, femoral artery thrombosis was first induced via topical application of FeCl_3_ (1). No accumulation of AF680-ProT was observed in the thrombus after injection of 25 ìg AF680-ProT. Endocarditis was then induced with the S. aureus strain that is deficient of both SC and vWbp (n = 10–13 mice). Only background levels of AF680-ProT accumulation were detected in the vegetations. Improved survival was also observed in these mice, suggesting that SC increases the virulence of S. aureus. Histology revealed leukocyte infiltration and the absence of the protective fibrin barrier in the vegetations induced by the SC and vWbp double-knockout S. aureus, indicating an impaired ability of the bacteria to evade the host defense. In the mice infected with an S. aureus strain that lacks only SC (n = 5 mice), AF680-ProT accumulation in the vegetations was reduced to 14% compared to mice that were infected with isogenic wild-type Newman strain bacteria (P < 0.0001).

Toxicity of the AF680-ProT was studied after three injections of 10 times (250 μg) the imaging dose over one week (n = 5 mice) (1). Pathological examination of the normal tissue sections revealed no abnormalities such as inflammatory foci, necrosis, clots, or bleeding. No differences were observed for the prothrombin time for either human or mouse plasma after incubation with the prothrombin analog (250 μg) at 37ºC. Tail tip bleeding assay also showed no significant changes in clotting parameters in mice injected with the probe (n = 5 mice).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently avaliable.

## References

1 Panizzi P., et al. (2011). In vivo detection of Staphylococcus aureus endocarditis by targeting pathogen-specific prothrombin activation. Nat Med.
2 Chorianopoulos E., et al. (2009). The role of endothelial cell biology in endocarditis. Cell Tissue Res.
3 Friedrich R., et al. (2003). Staphylocoagulase is a prototype for the mechanism of cofactor-induced zymogen activation. Nature.
4 Panizzi P., et al. (2004). The staphylocoagulase family of zymogen activator and adhesion proteins. Cell Mol Life Sci.
5 Hacisalihoglu A., et al. (2007). Restricted active site docking by enzyme-bound substrate enforces the ordered cleavage of prothrombin by prothrombinase. J Biol Chem.
6 Panizzi P., et al. (2006). Novel fluorescent prothrombin analogs as probes of staphylocoagulase-prothrombin interactions. J Biol Chem.
7 Panizzi P., et al. (2006). Fibrinogen substrate recognition by staphylocoagulase.(pro)thrombin complexes. J Biol Chem.
8 Friedrich R., et al. (2006). Structural basis for reduced staphylocoagulase-mediated bovine prothrombin activation. J Biol Chem.
9 Munnix I.C., et al. (2007). Segregation of platelet aggregatory and procoagulant microdomains in thrombus formation: regulation by transient integrin activation. Arterioscler Thromb Vasc Biol.
10 Watanabe S., et al. (2005). Structural comparison of ten serotypes of staphylocoagulases in Staphylococcus aureus. J Bacteriol.
11 Hirose M., et al. (2010). Identification of staphylocoagulase genotypes I-X and discrimination of type IV and V subtypes by multiplex PCR assay for clinical isolates of Staphylococcus aureus. Jpn J Infect Dis.